# Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Lys-polyethylene glycol-CGLIIQKNEC (CLT1)

Chemical name: | Gadolinium-1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Lys-polyethylene glycol-CGLIIQKNEC (CLT1)
Abbreviated name: | CLT1-dL-(Gd-DOTA)_4_
Synonym:
Agent category: | Peptide
Target: | Fibrin-fibronectin clot complexes
Target category: | Acceptor
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal/contrast: | Gadolinium, Gd
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal, and T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the development of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide nanoparticles and other iron oxide formulations affect T2 primarily and lead to decreased signals. On the other hand, paramagnetic T1 agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T1 relaxation and lead to brighter contrast images.

Extracellular matrix adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (2). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (3). A meshwork of clotted plasma protein was present in the tumor stroma but not in normal tissues, providing a functional matrix for angiogenesis, cell migration, and tumor cell invasion (4). There are high levels of collagens, fibronectin, and fibrin in the tumor connective tissues.

Gadolinium (Gd), a lanthanide metal ion with seven unpaired electrons, has been shown to be very effective in enhancing proton relaxation because of its high magnetic moment and water coordination (5, 6). Gd-Labeled diethylenetriamine pentaacetic acid (Gd-DTPA) was the first intravenous MRI contrast agent used clinically, and a number of similar Gd chelates have been developed in an effort to further improve clinical use. However, these low molecular weight Gd chelates have short blood and tissue retention times, which limit their use as imaging agents in the vasculature and cancer. Furthermore, they are largely nonspecific. CGLIIQKNEC (CLT1), a fibronectin-fibrin binding peptide, was identified with phage display screening (4). The peptide was conjugated with Gd-DTPA to form Gd-DTPA-CLT1 for imaging of fibronectin-fibrin complexes in tumor tissues showing specific accumulation in the tumors (7). Wu et al. (8) prepared a CLT1-targeted contrast agent (CLT1-dL-(Gd-DOTA)_4_) with four Gd-tetraazacyclododecane-1,4,7,10-tetraacetic acid (GD-DOTA) monoamide chelates conjugated to a CLT1 molecule via a generation 1 lysine dendrimer. CLT1-dL-(Gd-DOTA)_4_ was evaluated as a MRI tumor contrast agent in nude mice bearing orthotopic PC3 human prostate tumor.

### Related Resource Links:

- Chapters in MICAD (CLT1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CLT1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (fibrinogen (http://www.ncbi.nlm.nih.gov/gene/2243), fibronectin (http://www.ncbi.nlm.nih.gov/gene/2335))
- Articles in Online Mendelian Inheritance in Man (OMIM) (fibrinogen (http://www.ncbi.nlm.nih.gov/omim/134820), fibronectin (http://omim.org/entry/135600))
- Clinical trials (Gd-DTPA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DTPA), Gd-DOTA (http://www.clinicaltrials.gov/ct2/results?term=Gd-DOTA))
- Drug information in FDA (Gd-DTPA (http://google2.fda.gov/search?q=Gd-DTPA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1), Gd-DOTA (http://google2.fda.gov/search?q=Gd-DOTA&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&filter=1))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+synthesis)]

CLT1-dL-(DOTA)_4_ was synthesized with solid-phase synthesis (8). Polyethylene glycol (PEG), (Lys)_2_, and (DOTA)_4_ were sequentially conjugated to the N-terminus of the CLT1 peptide. The molecular weight (3,251.62) of CLT1-dL-(DOTA)_4_ was confirmed with MALDI-TOF mass spectroscopy. Gd(OAc)_3_ and CLT1-dL-(DOTA)_4_ were incubated at pH 6 for 48 h at room temperature. The product, CLT1-dL-(Gd-DOTA)_4_, was isolated with G-10 column chromatography. The mass (m/z, M + H^+^) of CLT1-dL-(Gd-DOTA)_4_ was 3,869.85 as determined with mass spectrometry (calculated: 3,869.53). A scrambled and inactive sCLT1-Gd-DOTA monoamide conjugate sCLT1-dL-(Gd-DOTA)_4_ was similarly prepared.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+in+vitro)]

CLT1-dL-(Gd-DOTA)_4_ exhibited r_1_ and r_2_ values of 40.4 ± 3.0 mM^–1^s^–1^ and 52.0 ± 9.6 mM^–1^s^–1^ at 1.5 T, respectively (8). sCLT1-dL-(Gd-DOTA)_4_ exhibited r_1_ and r_2_ values of 46.0 ± 5.0 mM^–1^s^–1^ and 49.6 ± 1.3 mM^–1^s^–1^ at 1.5 T, respectively. These values were higher than those of Gd-DOTA (2.9 and 3.2 mM^–1^s^–1^).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+rodentia)]

Wu et al. (8) performed dynamic T1-weighted MRI (7 T) studies with 0.03 mmol Gd/kg CLT1-dL-(Gd-DOTA)_4_ in mice (n = 6) bearing PC3 xenografts. sCLT1-dL-(Gd-DOTA)_4_ (0.03 mmol Gd/kg) was used a control contrast agent. sCLT1 is an inactive scrambled peptide. Contrast-enhanced MRI images were obtained before injection and at 1, 5, 10, 15, 20, 25, and 30 min after injection. Enhanced contrast in the tumor tissues and kidneys was visualized for CLT1-dL-(Gd-DOTA)_4_ at 1–30 min after injection. Contrast enhancement in the urinary bladder gradually increased over time. Kidney contrast was three-fold higher than the tumor contrast at 1 min. CLT1-dL-(Gd-DOTA)_4_ exhibited 110% greater enhancement in the tumors than sCLT1-dL-(Gd-DOTA)_4_ at 1 min, and 60% greater contrast enhancement at 30 min (P < 0.05). Both agents showed similar contrast enhancement in the kidneys with gradual washout. No blocking studies were performed.

Ex vivo biodistribution of Gd was studied in mice (n = 4/group) bearing PC3 xenografts at 48 h after injection of 0.03 mmol Gd/kg CLT1-dL-(Gd-DOTA)_4_ or sCLT1-dL-(Gd-DOTA)_4_ (8). The Gd retention values for both contrast agents were comparable in the heart, lung, liver, spleen, skin, and muscle (P > 0.05) but significantly different in the kidney, femur, and tumor (P < 0.05). The Gd contents were 0.5%, 0.8%, and 1.3% of injected dose of CLT1-dL-(Gd-DOTA)_4_ per gram of tissue (ID/g) in the liver, spleen, and kidney, respectively. The other tissues contained <0.1% ID/g. The tumor Gd contents were 0.05% ID/g and 0.01% ID/g for CLT1-dL-(Gd-DOTA)_4_ and sCLT1-dL-(Gd-DOTA)_4_, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=CLT1+human)]

No publication is currently available.

## NIH Support

R01 CA097465

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
3 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
4 Pilch J., Brown D.M., Komatsu M., Jarvinen T.A., Yang M., Peters D., Hoffman R.M., Ruoslahti E. (2006). Peptides selected for binding to clotted plasma accumulate in tumor stroma and wounds. Proc Natl Acad Sci U S A.
5 Brasch R.C. (1992). New directions in the development of MR imaging contrast media. Radiology.
6 Runge V.M., Gelblum D.Y. (1991). Future directions in magnetic resonance contrast media. Top Magn Reson Imaging.
7 Ye F., Wu X., Jeong E.K., Jia Z., Yang T., Parker D., Lu Z.R. (2008). A peptide targeted contrast agent specific to fibrin-fibronectin complexes for cancer molecular imaging with MRI. Bioconjug Chem.
8 Wu X., Burden-Gulley S.M., Yu G.P., Tan M., Lindner D., Brady-Kalnay S.M., Lu Z.R. (2012). Synthesis and Evaluation of a Peptide Targeted Small Molecular Gd-DOTA Monoamide Conjugate for MR Molecular Imaging of Prostate Cancer. Bioconjug Chem.